# ^89^Zr-N-Succinyldesferal-human anti-insulin-like growth factor 1 receptor monoclonal antibody R1507

Chemical name: | ^89^Zr-N-Succinyldesferal-human anti-insulin-like growth factor 1 receptor monoclonal antibody R1507
Abbreviated name: | ^89^Zr-R1507, ^89^Zr-Df-R1507
Synonym:
Agent category: | Antibody
Target: | Insulin-like growth factor 1 receptor (IGF-1R)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507)]

Insulin-like growth factor 1 (IGF-1, 70 amino acids) is secreted by the liver and target tissues in response to growth hormone stimulation (1). IGF-1 plays an important role in cell growth and development. IGF-1 binds to IGF-1 receptor (IGF-1R) with ~1,000-fold higher affinity than to insulin receptor. IGF-1R is a transmembrane tyrosine kinase receptor and is also highly expressed in many human cancers (2). IGF-1R plays an important role in tumor proliferation, apoptosis, angiogenesis, and metastasis (3, 4). Triple negative breast tumors are negative for estrogen receptors, progesterone receptors, and HER2. Patients with triple negative breast tumors have a lower survival rate than patients with estrogen receptor- or HER2-positive breast tumors (5). IGF-1R is overexpressed in 36% of all triple negative breast carcinomas (6). Therefore, monitoring of IGF-1R expression in breast tumor lesions with a non-invasive imaging modality is important for development of therapeutic treatments of these patients with anti-IGF-1R monoclonal antibodies (7). The human anti-IGF-1R monoclonal antibody R1507 is directed against the extracellular domain of human IGF-1R (8). In this chapter, Heskamp et al. (9) radiolabeled the human anti-IGF-1R monoclonal antibody R1507 with ^89^Zr for in vivo imaging of IFG-1R expression with positron emission tomography (PET). ^89^Zr-N-Succinyldesferal-human anti-IGF-1R monoclonal antibody R1507 (^89^Zr-R1507) has been evaluated in a triple negative breast cancer model in mice.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=IGF-1%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (IGF-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=3480)).
- Articles in Online Mendelian Inheritance in Man (OMIM) (IGF-1R (http://www.ncbi.nlm.nih.gov/omim/147370))
- Clinical trials (IGF-1R (http://www.clinicaltrials.gov/ct2/results?term=IGF1R))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20synthesis)]

R1507 was coupled with N-succinyldesferal via an amide linkage and labeled with ^89^Zr. R1507 was conjugated with two-fold molar excess of N-succinyldesferal-iron-tetrafluorophenol in 0.1 M NaHCO_3_ (pH 9) for 30 min at room temperature (9). A solution of 500 MBq (13.5 mCi) ^89^Zr and 3.3 nmol R1507 conjugate was incubated in buffer (pH 7.2) for 90 min at 35°C. ^89^Zr-R1507 was purified with column chromatography. ^89^Zr-R1507 exhibited a radiochemical purity of >98% with a labeling efficiency of 54%. The immunoreactivity of ^89^Zr-R1507 was not reported, whereas the immunoreactivity of ^111^In-DTPA-R1507 was 87%. The number of N-succinyldesferal groups per antibody was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20in%20vitro)]

Heskamp et al. (9) reported that the parent antibody R1507 exhibited 50% inhibitory concentration (IC_50_) values of 0.08–0.12 nM for IGF-1R on the triple negative human breast cancer cell line SUM149. ^111^In-DTPA-R1507 was mainly membrane-bound in the early hours of incubation and then was gradually internalized until 62% of the surface-bound radioactivity was internalized at 48 h after incubation. The in vitro internalization of ^89^Zr-R1507 in SUM149 cells was not reported

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20rodentia)]

Heskamp et al. (9) performed ex vivo biodistribution studies in nude mice (n = 6/group) bearing triple negative breast SUM149 xenografts with injection of 5.3 MBq (0.14 mCi, 66 pmol) ^89^Zr-R1507. Tumor accumulation was 22 ± 3% injected dose/gram (ID/g) at 7 d after injection. As a comparison, ^111^In-DTPA-R1507 showed tumor accumulation of 21 ± 3% ID/g at 7 d after injection. Blocking studies were performed only with ^111^In-DTPA-R1507, which showed >80% inhibition of IGF-1R binding.

PET imaging in nude mice showed that ^89^Zr-R1507 visualized the SUM149 tumor as early as 24 h after injection with a maximum contrast at 7 d. The tumor/liver ratios were 1.9 at 1 d, 2.9 at 3 d, and 4.7 at 7 d. Accumulation was observed in the liver, spleen, bone, and salivary glands. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=R1507%20and%20human)]

No publication is currently available.

## References

1 Hernandez-Sanchez C., Blakesley V., Kalebic T., Helman L., LeRoith D. (1995). The role of the tyrosine kinase domain of the insulin-like growth factor-I receptor in intracellular signaling, cellular proliferation, and tumorigenesis. J Biol Chem.
2 LeRoith D., Werner H., Neuenschwander S., Kalebic T., Helman L.J. (1995). The role of the insulin-like growth factor-I receptor in cancer. Ann N Y Acad Sci.
3 Rosenzweig S.A., Atreya H.S. (2010). Defining the pathway to insulin-like growth factor system targeting in cancer. Biochem Pharmacol.
4 Baserga R., Hongo A., Rubini M., Prisco M., Valentinis B. (1997). The IGF-I receptor in cell growth, transformation and apoptosis. Biochim Biophys Acta.
5 Carey L.A., Dees E.C., Sawyer L., Gatti L., Moore D.T., Collichio F., Ollila D.W., Sartor C.I., Graham M.L., Perou C.M. (2007). The triple negative paradox: primary tumor chemosensitivity of breast cancer subtypes. Clin Cancer Res.
6 Lerma E., Peiro G., Ramon T., Fernandez S., Martinez D., Pons C., Munoz F., Sabate J.M., Alonso C., Ojeda B., Prat J., Barnadas A. (2007). Immunohistochemical heterogeneity of breast carcinomas negative for estrogen receptors, progesterone receptors and Her2/neu (basal-like breast carcinomas). Mod Pathol.
7 Zha J., O'Brien C., Savage H., Huw L.Y., Zhong F., Berry L., Lewis Phillips G.D., Luis E., Cavet G., Hu X., Amler L.C., Lackner M.R. (2009). Molecular predictors of response to a humanized anti-insulin-like growth factor-I receptor monoclonal antibody in breast and colorectal cancer. Mol Cancer Ther.
8 Gong Y., Yao E., Shen R., Goel A., Arcila M., Teruya-Feldstein J., Zakowski M.F., Frankel S., Peifer M., Thomas R.K., Ladanyi M., Pao W. (2009). High expression levels of total IGF-1R and sensitivity of NSCLC cells in vitro to an anti-IGF-1R antibody (R1507). PLoS One.
9 Heskamp S., van Laarhoven H.W., Molkenboer-Kuenen J.D., Franssen G.M., Versleijen-Jonkers Y.M., Oyen W.J., van der Graaf W.T., Boerman O.C. (2010). ImmunoSPECT and immunoPET of IGF-1R expression with the radiolabeled antibody R1507 in a triple-negative breast cancer model. J Nucl Med.